# [^18^F]Y1-973

Chemical name: | [^18^F]Y1-973
Abbreviated name: | [^18^F]Y1-973
Synonym:
Agent category: | Compound
Target: | Neuropeptide Y receptor Y1 (NPY1R)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Non-human primates | Click on protein (http://www.ncbi.nlm.nih.gov/protein/NP_000900.1), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_000909.5) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=4886) for more information about neuropeptide Y receptor Y1 (NPY1R).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Y1-973)]

Neuropeptide Y (NPY; 36 amino acids) is one of the most abundant neuropeptides in the mammalian central nervous system, and it is produced in the arcuate and dorsomedial hypothalamic nuclei (1). NPY exhibits a diverse range of important physiological activities, including effects on psychomotor activity, food intake, regulation of central endocrine secretion, and energy homeostasis, as well as potent vasoactive effects on the cardiovascular system. High levels of NPY are found in the striatum, nucleus accumbens, amygdala, frontal cortex, hypothalamus, and hippocampus (2). Five subtypes of NPY (Y1, Y2, Y4, Y5, and Y6) have been defined by pharmacological criteria (3). The Y2 and Y4 receptor subtypes are thought to inhibit appetite, whereas the Y1 and Y5 receptor subtypes are responsible for stimulation of appetite. NPY receptors, such as NPY1R, have been identified in a variety of tissues, including the brain, spleen, small intestine, kidney, testis, placenta, and aortic smooth muscle (4). Kameda et al. (5) reported a series of 2,4-diaminopyridine small molecule NPY1R-selective antagonists with properties that are attractive for brain imaging. One of these antagonists, Y1-973, is reported to have IC_50_ values of 0.13 nM for human NPY1R and >10,000 nM for human NPY2R, NPY4R, and NPY5R. Y1-973 is not a substrate for the human P-glycoprotein transporter. Y1-973 was radiolabeled with ^18^F as [^18^F]Y1-973 for use with positron emission tomography (PET) imaging of NPY1R expression, and [^18^F]Y1-973 has been evaluated in rhesus monkey brain (6). [^18^F]Y1-973 showed good brain accumulation, with regional heterogeneity and specific binding to NPY1R in vivo in monkeys.

### Related Resource Links:

- Chapters in MICAD (NPY1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Neuropeptide%20Y%20%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (NPY (http://www.ncbi.nlm.nih.gov/gene/4852), NPY1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=4886))
- Articles in Online Mendelian Inheritance in Man (OMIM) (NPY (http://omim.org/entry/162640), NPY1R (http://omim.org/entry/162641))
- Clinical trials (NPY (http://www.clinicaltrials.gov/ct2/results?term=neuropeptide+y&Search=Search), NPY1R (http://www.clinicaltrials.gov/ct2/show/NCT01387724?term=Neuropeptide+Y+receptor&rank=1))
- Drug information in FDA (NPY (http://google2.fda.gov/search?q=neuropeptide+Y&client=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&sort=date%3AD%3AL%3Ad1&entqr=3&entqrm=0&oe=UTF-8&ie=UTF-8&ud=1&site=FDAgov&filter=1&btnG=Search), NPY1R (http://google2.fda.gov/search?q=neuropeptide+Y+receptor&client=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&sort=date%3AD%3AL%3Ad1&entqr=3&entqrm=0&oe=UTF-8&ie=UTF-8&ud=1&site=FDAgov&filter=1&btnG=Search))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Y1-973%20and%20synthesis)]

The radiosynthesis of [^18^F]Y1-973, reported by Hostetler et al. (6), involved standard fluoronucleophilic substitution of the corresponding chloride precursor with K[^18^F]F/Kryptofix2.2.2 in dimethyl sulfoxide for 2 min at 130°C, followed by HCl hydrolysis to remove the Boc-protecting group (5 min, 130°C). The reported overall radiochemical yield of the radiosynthesis was 18 ± 13%, the specific activities were 41.8 ± 23.2 GBq/mmol (1,548 ± 859 mCi/mmol) at the end of synthesis (EOS), and the radiochemical purity was >98%. The total synthesis time was 45 min. The log P value for [^18^F]Y1-973 was 3.2 (lipophilic).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Y1-973%20and%20in%20vitro)]

Hostetler et al. (6) performed in vitro autoradiography studies with [^18^F]Y1-973 in monkey and human brain tissue. The highest radioactivity was observed in the hippocampal dentate gyrus, caudate-putamen and cortical cingulate, followed by moderate radioactivity in the hypothalamus and thalamus. Low radioactivity was observed in the globus pallidus and cerebellum, a region poor in NPY receptors. Unlabeled Y1-973 blocked the radioactivity levels in all brain regions to background level.

Saturation binding studies in frontal cortex and caudate putamen tissue from monkey and human brains were performed with [^3^H]Y1-973 (6). Nonlinear curve-fitting analyses identified two binding sites in these regions for both species. The high-affinity binding sites had K_d_ values of 0.06–0.1 nM. The low-affinity binding sites had K_d_ values of 8–25 nM for the frontal cortex and 78–148 nM and for the caudate putamen. The binding potential (BP) values were 39–49 for the high-affinity binding site and 1.7–3.4 for the low-affinity binding site.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Y1-973%20and%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Y1-973%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Y1-973%20and%20%28primate%20not%20human%29)]

Dynamic PET imaging studies were performed in rhesus monkeys (n = 2) for 90 min after intravenous injection of [^18^F]Y1-973 (amount of radioactivity not reported) (6). High initial accumulation (5 min after injection) was observed in the brain, with heterogeneous distribution. The highest accumulation was observed at 30 min in the striatum, followed by the cortical regions, thalamus, pons, and cerebellum. The radioactivity level in the striatum peaked at ~30 min and slowly decreased thereafter, whereas radioactivity levels in other brain regions declined gradually after their peak accumulation at 5 min. Logan graphical analyses of the two monkeys showed that the highest BP values were in the striatum (1.79 and 2.01), followed by the parietal cortex (1.44 and 1.62), occipital cortex (1.05 and 0.87), thalamus (0.62 and 0.63), and cerebellum (0.44 and 0.33). A displacement study was performed with injection of 2.5 mg/kg Y1-718 (selective NPY1R antagonist, IC_50_ = 17 nM) 30 min after injection of [^18^F]Y1-973. An increase of radioactivity clearance in the striatum was observed within a few min of Y1-718 injection, whereas little change was observed in the cerebellum. Blocking studies were performed with injection of 2.7 mg/kg plus infusion (1.8 mg/kg/h) or 8.1 mg/kg plus infusion (5.4 mg/kg/h) Y1-718 immediately after injection of [^18^F]Y1-973. The low and high doses of Y1-718 resulted in a notable decrease in accumulation of [^18^F]Y1-973 in the striatum and cortical regions, with 74% and 93% receptor occupancy, respectively.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Y1-973%20and%20human)]

No publication is currently available.

## References

1 Decressac M., Barker R.A. (2012). Neuropeptide Y and its role in CNS disease and repair. Exp Neurol.
2 Adrian T.E., Allen J.M., Bloom S.R., Ghatei M.A., Rossor M.N., Roberts G.W., Crow T.J., Tatemoto K., Polak J.M. (1983). Neuropeptide Y distribution in human brain. Nature.
3 Larhammar D., Wraith A., Berglund M.M., Holmberg S.K., Lundell I. (2001). Origins of the many NPY-family receptors in mammals. Peptides.
4 Herzog H., Hort Y.J., Ball H.J., Hayes G., Shine J., Selbie L.A. (1992). Cloned human neuropeptide Y receptor couples to two different second messenger systems. Proc Natl Acad Sci U S A.
5 Kameda M., Ando M., Nakama C., Kobayashi K., Kawamoto H., Ito S., Suzuki T., Tani T., Ozaki S., Tokita S., Sato N. (2009). Synthesis and evaluation of a series of 2,4-diaminopyridine derivatives as potential positron emission tomography tracers for neuropeptide Y Y1 receptors. Bioorg Med Chem Lett.
6 Hostetler E.D., Sanabria-Bohorquez S., Fan H., Zeng Z., Gantert L., Williams M., Miller P., O'Malley S., Kameda M., Ando M., Sato N., Ozaki S., Tokita S., Ohta H., Williams D., Sur C., Cook J.J., Burns H.D., Hargreaves R. (2011). Synthesis, characterization, and monkey positron emission tomography (PET) studies of [18F]Y1-973, a PET tracer for the neuropeptide Y Y1 receptor. Neuroimage.